# Gadolinium-1,4,7,10-tetraazacyclododecane-N,N’,N’,N’”-tetraacetic-monoamide-24-cascade-polymer

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-N,N’,N”,N’”-tetraacetic-monoamide-24-cascade-polymer
Abbreviated name: | 24GdDOTACP
Synonym: | Gadomer-17®, SHL 643A
Agent category: | Small molecule
Target: | Other
Target category: | Other – blood pool agent
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gadomer+17)]

Magnetic resonance imaging (MRI) delineates soft tissues by sampling the signal of tissue water protons to detect abnormalities in anatomy, pathology, and functionality in the human body. The imaging contrast, defined as the relative brightness of various parts of the body, is primarily determined by the tissue structures and the spin relaxation times of the water protons (the longitudinal relaxation time (T_1_) and the transverse relaxation time (T_2_)). Many physiological processes, including blood flow, diffusion, perfusion, and chemical exchange, also affect the imaging contrast. To improve the imaging contrast, a variety of experimental parameters can be optimized. Imaging contrast can be improved locally by using contrast agents specifically targeted to tissues and organs (1, 2). Blood pool agents are paramagnetic contrast agents designed to remain in the blood for a prolonged time compared to the conventional contrast agents like gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA). Blood pool agents are normally macromolecules attached gadolinium chelates or iron oxide nanoparticles (1).Their large size prevents them from diffusing through the endothelium of normal tissue and entering into interstitial space in detectable amounts before being completely excreted from body. In addition to the applications in magnetic resonance angiography (3-5), blood pool agents are used to target necrotic myocardium (6, 7), to access myocardial viability (8), and to detect various tumors (9, 10).

24-Gadolinium-1,4,7,10-tetraazcyclododecane-N,N’,N”,N”’-tetraacetic monoamide (GdDOTA)_24_-cascade-polymer is a synthetic polymeric gadolinium complex designed as a blood pool contrast agent for MRI (11, 12). The main molecular frame is a dendritic structure (dendrimer) built from a tri-mesoyl[benzene-1,3,5-tricarbonyl] core surrounded by two generations of 6 and 12 L-lysine residues. 24 gadolinium-1,4,7,10-tetraazcyclododecane-N,N’,N”,N”’-tetraacetic monoamide (Gd-DOTA) moieties are covalently bound at the molecular surface (12, 13). Each Gd-DOTA moiety contains lanthanide Gd(III) of high electron spin (7/2) and long electron relaxation time (14). Gd(III) forms a very stable complex with DOTA and leaves one structural water in rapid exchange with the bulk water of tissues. As a result, the T_1_ relaxation time of tissue water protons reduces significantly. DOTA is a macrocyclic and can form a stable complex with Gd(III). Gd-DOTA has an in vitro stability five orders of magnitude greater than that of Gd-DTPA (14). This greater stability allows for reduction of the in vivo toxicity caused by the dissociation of free Gd(III) in the metabolic process (14). Attaching Gd-DOTA to a macromolecule generates a field-dependent paramagnetic enhancement effect (PRE) (15, 16). The efficacy increases substantially as a result of the increase of the effective rotation correlation time τ_R_. The synthesis of dendrimer starts with formation of a core. Monomers are assembled radially according to certain dendritic rules and cascade to higher generations like a starburst. Dendrimers built in this way have a globular shape, which provides an open surface for attaching various species such as imaging agents and therapeutic drugs (17). As a carrier for MRI contrast agents, dendrimers possess a mono-dispersed, well-defined, and stable molecular structure with rigid branch segments, allowing the synthesis of paramagnetic particles with well-defined size and efficacy (17, 18). (GdDOTA)_24_-cascade-polymer is a blood pool agent of intermediate size that can effectively delineate small vessels, detect capillary permeability, improve myocardial ischemia detections, estimate blood flow and blow volume, and characterize tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadomer+17)+AND+synthesis)]

Nicolle et al. described a detailed synthesis of the dendritic backbone of free 24mer amine (13). First the monomer N,N’-(iminodi-2,1-ethandiyl)-bis[N2,N6-bis[(benzyloxy)carbonyl]-L-lysinamide) was prepared in a single step from commercially available starting materials. Three equivalents of the monomer were then reacted with the central core benzene-1,3,5-tricarbonyl trichloride to produce the benzyloxycarbonyl-protected 12mer amines with 80% yield. This procurer was converted to the free 12mer amine and subsequently treated with N_a_,N_t_-dibenzyloxy-carbonyl-L-lysine-p-nitrophenyl ester to produce the protected 24mer amine with >80% yield. The protected 24mer was further converted to the free 24mer amine (13). Coupling of a three-fold molar excess p-nitrophenyl ester of DOTA with the free 24mer amine generated dendritic DOTA ligand, followed by complexation with Gd_2_O_3_ to form (GdDOTA)_24_-cascade-polymer (13). This compound has 24 GdDOTAs and the molecular mass is 17.753 kDa. Because the compound has a globular shape, the apparent molecular weight is 30–35 kDa (12). (GdDOTA)_24_-cascade-polymer is commercially available (Schering AG, Berlin, Germany) and is currently undergoing phase II clinical trials (19, 20).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadomer)+and+(in+vitro))]

The relaxivities of (GdDOTA)_24_-cascade-polymer in water or blood plasma were measured at several magnetic field strengths and temperatures (11, 12). The T_1_ relaxivity in water was 17.3 ± 0.1 mmol Gd^-1^ • s^-1^ at 0.47 T (20 MHz) at 39°C and 12.6 ± 0.1 mmol Gd^-1^ • s^-1^ at 2 T (85 Hz) at 22°C. In blood plasma, the T_1_ relaxivity increased slightly to 18.3 ± 0.4 mmol Gd^-1^ • s^-1^ and 13.5 ± 0.1 mmol Gd^-1^ • s^-1^, respectively. In comparison, the T_1_ relaxivity of GdDOTA in water was 3.84 mmol Gd^-1^ • s^-1^ at 0.47 T. The T_2_ relaxivity was higher than the T_1_ relaxivity. In water, the T_2_ relaxivity was 22.4 ± 0.1 mmol Gd^-1^ • s^-1^ at 0.47 T and 20.0 ± 0.1 mmol Gd^-1^ • s^-1^ at 2 T, and increased to 29.3 ± 2.3 mmol Gd^-1^ • s^-1^ and 21.4 ± 0.3 mmol Gd^-1^ • s^-1^ in plasma, respectively. The osmolality and viscosity at 0.5 mol/L at 37°C were measured to be 0.38 (osmol/kg) and 7 mPa/s, respectively (11).

The relaxation properties of water were examined with ^1^H nuclear magnetic resonance (NMR) dispersion spectroscopy (NMRD) at different magnetic field strengths and with ^17^O NMR spectroscopy at different temperatures (13). The electron spin relaxation rates of Gd(III) were examined with electron paramagnetic resonance (EPR) spectrometers at three operating frequencies (9.4, 150, and 225 GHz) (13). Three types of kinetic parameters that determine the relaxation rate constant were calculated from these measurements. The water exchange kinetic rate constant (k_ex_) was calculated to be 1.0 x 10^6^ s^-1^ at 25°C. This value is very similar to those found for gadolinium DOTA-monoamide derivatives. The local and the global rotation correlation times (τ_s_ and τ_g_) for the bound Gd-DOTA moieties were found to be 760 ± 120 ps and 3,050 ± 250 ps, respectively. The electron relaxation time τ_v_ was found to be 46 ± 3 ps at 25°C (13).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadomer+17)+AND+rodentia)]

The pharmacokinetic study in rats was conducted at a dose of 0.1 mmol Gd/kg (12). The concentration in blood plasma was measured by gamma (γ) counting of the radioactive ^153^Gd-labeled (GdDOTA)_24_-cascade-polymer after a bolus injection. The elimination from the blood was biphasic in the rats with a total plasma clearance of 8.1 ml/min per kg. The half-life was 2 min for the initial arterial phase with a blood volume (Vc) of 0.04 L/kg and 37 min for the steady-state phase with a total blood volume (Vss) of 0.13 L/kg.

The biodistribution in rats was investigated at 24 h, 7 days, and 14 days after an intravenous injection of the ^153^Gd-labeled (GdDOTA)_24_-cascade-polymer at a dose of 0.1 mmol Gd/kg (12). About 80% of the injected dose (ID) was excreted in the first hour in urine as (GdDOTA)_24_-cascade-polymer, and 91% ID in the first day. Fecal elimination was <1%. At 14 days after injection, only 0.12% ID was detected in the kidney, 0.04% in the liver, 0.04% in the gastrointestinal tract, and 0.50% in the carcass. The acute systemic tolerance LD_50_ after a single intravenous injection was found to be ≥20 mmol/kg in rats (21) and ≥30 mmol Gd/kg in mice (12).

The extravasation properties associated with leaky vasculatures were measured in hamsters bearing amelanotic melanomas (22). Fluorescein isothiocyanate (FITC)-labeled (GdDOTA)_24_-cascade-polymer was administrated intravenously at a dose of 0.2 mmol/kg. An in vivo fluorescence microscopy was used to examine the tumors in the dorsal skin fold chamber. (GdDOTA)_24_-cascade-polymer was found to leak into the interstitial space in the area of neovascularized tumors immediately after injection and into the tumor-free tissues in the area with neoplastic tumor 5 min later. Dynamic MRI permitted the calculation of the rate for the agents leaking into the interstitial space after a bolus injection. This rate as a measure of vascular permeability was used to differentiate various tumors in rodent models (23-26). The applications included lymph node tumor metastasis (23), gliomas (24), malignant breast tumors (25), infiltrating ductal carcinomas (26), R3230 AC adenocarinomas (21), human skin HaCaT-ras-A-5RT3 carcinomas, and prostate R3327-AT1 carcinomas (27). (GdDOTA)_24_-cascade-polymer was also used in a study of myocardial diseases for delineation of very small microvascular obstructions in ischemically injured myocardium of rats (28).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

A pharmacokinetic study was also carried out in rabbits at a dose of 0.05 mmol Gd/kg and in dogs at a dose of 0.1 mmol Gd/kg (12). The concentration in blood plasma was measured by gamma (γ) counting of the radioactive ^153^Gd-labeled (GdDOTA)_24_-cascade-polymer after a bolus injection. Elimination from blood was biphasic, and the total plasma clearance was 4.4 ml/min per kg in the rabbits and 3.5 ml/min per kg in the dogs. The half-life in the rabbits was 4 min for the arterial phase with Vc of 0.041 L/kg and 28 min for the steady-state phase with Vss of 0.10 L/kg. The half-life in the dogs was 11 min for the arterial phase with Vc of 0.071 L/kg and 110 min for the steady-state phase with Vss of 0.19 L/kg.

Dong et al. measured the enhancement effects in abdominal and thoracic MR angiography in dogs at five doses (0.01, 0.025, 0.05, 0.1, and 0.2 mmol Gd/kg) (11). The signal-to-noise ratio increased at doses >0.01 mmol/kg and was found in aorta, inferior vena cava, portal vein, renal arteries and veins, celiac trunk, superior mesenteric artery, and pulmonary arteries and veins. The signal-to-noise was three-fold greater in the aorta in the arterial phase and four-fold greater in the aorta and the inferior vena cava in the steady-state phase in comparison with that of small Gd-chelates. Clarke et al. studied the steady-state phase angiography properties of (GdDOTA)_24_-cascade-polymer in the aorta of health rabbits at four doses (0.015, 0.025, 0.05, and 0.1 mmol Gd/kg) (29). The enhancement was also tested in the pulmonary MR angiography in pigs (30, 31) and in the coronary angiography in pigs (32) and cats (33).

Misselwitz et al. studied the interstitial MR lymphography in dogs at three doses (0.001, 0.0025, and 0.01 mmol/kg) on a 1.5-T MR imager (34). With a dose >0.0025 mmol/kg, the enhancement of 120–168% occurred 15 min after injection. Depending on the dosage, the maximum signal increase ranging from 450–960% was observed at 60–90 minutes after injection. Torchia et al. performed the detection of the sentinel lymph nodes in pigs by dynamic MR lymphangiography on a 0.2-T MR imager (35). (GdDOTA)_24_-cascade-polymer was also used to evaluated the effects of various treatments of VX2 carcinomas in rabbits models, such as radio frequency ablations (36) and x-ray irradiations (37).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadomer+17)+AND+(primate+not+human))]

A pharmacokinetic study was also performed in cynomolgus monkeys at a dose of 0.1 mmol Gd/kg (12). The concentration in blood plasma was measured by gamma (γ) counting of the radioactive ^153^Gd-labeled (GdDOTA)_24_-cascade-polymer after a bolus injection. The elimination from the blood was biphasic in the monkeys with a total plasma clearance of 4.3 ml/min per kg. The half-life was 9 min for the initial arterial phase with Vc of 0.06 L/kg and 168 min for the steady-state phase with Vss of 0.21 L/kg.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(gadomer+17)+AND+human)]

Herborn et al. conducted MR angiography of coronary arteries in 12 healthy male volunteers (age range, 26–36 years; average age, 32.3 years) (19). Fast T_1_-weighted, three-dimensional, gradient-echo images were acquired with a 1.5-T MR imager at a dose of 0.1 mmol Gd/kg. The study was further extended to the patients with angiographically proven coronary artery disease (20). Twelve patients (seven men, five women; age range, 47–78 years; average age, 61.3 years) with luminal narrowing >50% were examined with the same imaging protocols. No significant changes in pulse rate, arterial blood pressure, oxygen saturation, hematology, and urinalysis were found for both groups after the injection. Satisfactory tolerance was reported for all participants without acute or later-phase adverse effects. The blood to myocardium contrast-to-noise ratio increased significantly in the 30 minutes after injection and led to a considerable improvement in the imaging qualities.

### NIH Support

HL38698, CA82923,

## References

1 Weinmann H.J., Ebert W., Misselwitz B., Schmitt-Willich H. (2003). Tissue-specific MR contrast agents. Eur J Radiol.
2 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
3 Fink C., Goyen M., Lotz J. (2007). Magnetic resonance angiography with blood-pool contrast agents: future applications. Eur Radiol.
4 Kramer H., Morana G. (2007). Whole-body magnetic resonance angiography with blood-pool agents. Eur Radiol.
5 Hoffmann U., Schima W., Herold C. (1999). Pulmonary magnetic resonance angiography. Eur Radiol.
6 Kroft L.J., de Roos A. (1999). Blood pool contrast agents for cardiovascular MR imaging. J Magn Reson Imaging.
7 Muhler A. (1995). Assessment of myocardial perfusion using contrast-enhanced MR imaging: current status and future developments. Magma.
8 Schmiedl U., Moseley M.E., Sievers R., Ogan M.D., Chew W.M., Engeseth H., Finkbeiner W.E., Lipton M.J., Brasch R.C. (1987). Magnetic resonance imaging of myocardial infarction using albumin-(Gd-DTPA), a macromolecular blood-volume contrast agent in a rat model. Invest Radiol.
9 Kiessling F., Morgenstern B., Zhang C. (2007). Contrast agents and applications to assess tumor angiogenesis in vivo by magnetic resonance imaging. Curr Med Chem.
10 Daldrup H.E., Roberts T.P., Muhler A., Gossmann A., Roberts H.C., Wendland M., Rosenau W., Brasch R.C. (1997). , and , .
11 Dong Q., Hurst D.R., Weinmann H.J., Chenevert T.L., Londy F.J., Prince M.R. (1998). Magnetic resonance angiography with gadomer-17. An animal study original investigation. Invest Radiol.
12 Misselwitz B., Schmitt-Willich H., Ebert W., Frenzel T., Weinmann H.J. (2001). Pharmacokinetics of Gadomer-17, a new dendritic magnetic resonance contrast agent. Magma.
13 Nicolle G.M., Toth E., Schmitt-Willich H., Raduchel B., Merbach A.E. (2002). The impact of rigidity and water exchange on the relaxivity of a dendritic MRI contrast agent. Chemistry.
14 Bousquet J.C., Saini S., Stark D.D., Hahn P.F., Nigam M., Wittenberg J., Ferrucci J.T. (1988). Gd-DOTA: characterization of a new paramagnetic complex. Radiology.
15 Lauffer R.B. (1987). Paramagnetic metal complexes as water proton relaxation agents for NMR imaging:Theory and design. Chem. Rev.
16 Caravan P., Ellison J.J., McMurry T.J., Lauffer R.B. (1999). Gadolinium(III) Chelates as MRI Contrast Agents: Structure, Dynamics, and Applications. Chem Rev.
17 Svenson S., Tomalia D.A. (2005). Dendrimers in biomedical applications--reflections on the field. Adv Drug Deliv Rev.
18 Wiener E.C., Brechbiel M.W., Brothers H., Magin R.L., Gansow O.A., Tomalia D.A., Lauterbur P.C. (1994). Dendrimer-based metal chelates: a new class of magnetic resonance imaging contrast agents. Magn Reson Med.
19 Herborn C.U., Barkhausen J., Paetsch I., Hunold P., Mahler M., Shamsi K., Nagel E. (2003). Coronary arteries: contrast-enhanced MR imaging with SH L 643A--experience in 12 volunteers. Radiology.
20 Herborn C.U., Schmidt M., Bruder O., Nagel E., Shamsi K., Barkhausen J. (2004). MR coronary angiography with SH L 643 A: initial experience in patients with coronary artery disease. Radiology.
21 Su M.Y., Wang Z., Nalcioglu O. (1999). Investigation of longitudinal vascular changes in control and chemotherapy-treated tumors to serve as therapeutic efficacy predictors. J Magn Reson Imaging.
22 Schneider G., Seidel R., Uder M., Wagner D., Weinmann H.J., Kramann B. (2000). In vivo microscopic evaluation of the microvascular behavior of FITC-labeled macromolecular MR contrast agents in the hamster skinfold chamber. Invest Radiol.
23 Kobayashi H., Kawamoto S., Choyke P.L., Sato N., Knopp M.V., Star R.A., Waldmann T.A., Tagaya Y., Brechbiel M.W. (2003). Comparison of dendrimer-based macromolecular contrast agents for dynamic micro-magnetic resonance lymphangiography. Magn Reson Med.
24 Verhoye M., van der Sanden B.P., Rijken P.F., Peters H.P., Van der Kogel A.J., Pee G., Vanhoutte G., Heerschap A., Van der Linden A. (2002). Assessment of the neovascular permeability in glioma xenografts by dynamic T(1) MRI with Gadomer-17. Magn Reson Med.
25 Daldrup-Link H.E., Shames D.M., Wendland M., Muhler A., Gossmann A., Rosenau W., Brasch R.C. (2000). Comparison of Gadomer-17 and gadopentetate dimeglumine for differentiation of benign from malignant breast tumors with MR imaging. Acad Radiol.
26 Su M.Y., Wang Z., Carpenter P.M., Lao X., Muhler A., Nalcioglu O. (1999). Characterization of N-ethyl-N-nitrosourea-induced malignant and benign breast tumors in rats by using three MR contrast agents. J Magn Reson Imaging.
27 Fink C., Kiessling F., Bock M., Lichy M.P., Misselwitz B., Peschke P., Fusenig N.E., Grobholz R., Delorme S. (2003). High-resolution three-dimensional MR angiography of rodent tumors: morphologic characterization of intratumoral vasculature. J Magn Reson Imaging.
28 Krombach G.A., Higgins C.B., Chujo M., Saeed M. (2005). Gadomer-enhanced MR imaging in the detection of microvascular obstruction: alleviation with nicorandil therapy. Radiology.
29 Clarke S.E., Weinmann H.J., Dai E., Lucas A.R., Rutt B.K. (2000). Comparison of two blood pool contrast agents for 0.5-T MR angiography: experimental study in rabbits. Radiology.
30 Nael K., Saleh R., Nyborg G.K., Fonseca C.G., Weinmann H.J., Laub G., Finn J.P. (2007). Pulmonary MR perfusion at 3.0 Tesla using a blood pool contrast agent: Initial results in a swine model. J Magn Reson Imaging.
31 Abolmaali N.D., Hietschold V., Appold S., Ebert W., Vogl T.J. (2002). Gadomer-17-enhanced 3D navigator-echo MR angiography of the pulmonary arteries in pigs. Eur Radiol.
32 Li D., Zheng J., Weinmann H.J. (2001). Contrast-enhanced MR imaging of coronary arteries: comparison of intra- and extravascular contrast agents in swine. Radiology.
33 Lee S.S., Goo H.W., Park S.B., Lim C.H., Gong G., Seo J.B., Lim T.H. (2003). MR imaging of reperfused myocardial infarction: comparison of necrosis-specific and intravascular contrast agents in a cat model. Radiology.
34 Misselwitz B., Schmitt-Willich H., Michaelis M., Oellinger J.J. (2002). Interstitial magnetic resonance lymphography using a polymeric t1 contrast agent: initial experience with Gadomer-17. Invest Radiol.
35 Torchia M.G., Misselwitz B. (2002). Combined MR lymphangiography and MR imaging-guided needle localization of sentinel lymph nodes using Gadomer-17. AJR Am J Roentgenol.
36 Moon W.K., Chang K.H., Weinmann H.J., Koh Y.H., Im J.G., Yeon K.M., Han M.C. (2000). Dynamic contrast-enhanced MR imaging of bacterial abscess and VX2 carcinoma in rabbits: comparison of gadopentetate dimeglumine and a macromolecular contrast agent. AJR Am J Roentgenol.
37 Kim Y.H., Choi B.I., Cho W.H., Lim S., Moon W.K., Han J.K., Weinmann H.J., Chang K.H. (2003). Dynamic contrast-enhanced MR imaging of VX2 carcinomas after X-irradiation in rabbits: comparison of gadopentetate dimeglumine and a macromolecular contrast agent. Invest Radiol.